# Ultrasmall superparamagnetic iron oxide nanoparticles conjugated with Ile-Pro-Leu-Pro-Phe-Tyr-Asn

Chemical name: | Ultrasmall superparamagnetic iron oxide nanoparticles conjugated with Ile-Pro-Leu-Pro-Phe-Tyr-Asn
Abbreviated name: | USPIO-PHO
Synonym:
Agent category: | Peptide
Target: | ß-amyloid (Aß_42_) peptide
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific molecular imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (2). It is characterized pathologically by neuronal loss with the presence in the brain of senile plaques of β-amyloid (Aβ) peptides and intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD. Early diagnosis of AD is important for treatment consideration and disease management (5). Several radioligands for positron emission tomography have been developed (6-8) and tested in humans as in vivo diagnostic tools for molecular imaging and measuring the formation of Aβ deposits (8). USPIO is composed of iron nanoparticles 4–6 nm in diameter, and the hydrodynamic diameter with polyethylene glycol or dextran coating is 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life of plasma relaxation times is calculated at ~24 h in humans (9) and 2 h in mice (10). Because of its long blood half-life, USPIO can be used as a blood pool agent during the early phase of intravenous administration (11). In the late phase, USPIO is suitable for the evaluation of RES in the body, particularly in lymph nodes (12). A cyclic peptide, Cys-Ile-Pro-Leu-Pro-Phe-Tyr-Asn-Cys, was identified with phage screening against Aβ_42_ peptide (13). Ile-Pro-Leu-Pro-Phe-Tyr-Asn (PHO) was synthesized and conjugated to dextran-coated USPIO to form USPIO-PHO for MRI of Aβ_42_ in the brain.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid)
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20synthesis)]

PHO peptide was linked covalently to USPIO with the reactive alkyl halogen end of epichlohydrin binding to the hydroxyls of dextran coating of Fe_3_O_4_ particles (USPIO) to obtain a terminal glycidyl ether derivatives, which were then reacted with the amine group of the peptide (13). Longitudinal (r_1_) and transverse (r_2_) relaxivities (nuclear magnetic resonance (NMR) efficiency expressed in s−^1^mM−^1^) of USPIO-PHO were measured at 37°C and 20 MHz (r_1_ = 32.26, r_2_ = 85.32, and r_2_/r_1_ = 2.64) and 60 MHz (r_1_ = 13.50, r_2_ = 83.75, and r_2_/r_1_ = 6.20). The number of PHO peptides per USPIO was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20in%20vitro)]

Larbanoix et al. (13) performed in vitro binding of USPIO-PHO to mouse Aβ_42_. USPIO-PHO had a binding affinity of 0.12 nM as determined with NMR relaxometry. USPIO did not bind to mouse Aβ_42_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20rodentia)]

Larbanoix et al. (13) performed ex vivo biodistribution in rats (n = 3/group) after injection of UPSIO-PHO or USPIO. UPSIO-PHO (0.1 mmol Fe/kg) had a blood half-life for elimination of 779 min, which was longer than that of USPIO (255 min). A majority of iron was found in the lungs and liver for both nanoparticles. There was a significant contrast enhancement of USPIO-PHO in the brain compared to USPIO (P < 0.05). In another experiment, USPIO-PHO nanoparticles (0.08 mmol Fe/kg) were injected intravenously to a double transgenic APP/PS1 mouse after injection of 25% mannitol to open up the brain–blood barrier. MRI imaging was performed at 4.7 T. There was a signal decrease of 48% in the cortex and striatum areas at 9 min, and the signal stayed constant up to 87 min after injection of the nanoparticles. In contrast, there was only ~15% maximum signal decrease in these brain areas in the wild-type mouse at 32 min after injection. Histological staining of Fe in the brain sections of APP/PS1 mice showed that there was a large amount of Fe in the brain section incubated with USPIO-PHO but not with USPIO. The Fe staining colocalized with the core of neuritic plaques (Sirius red staining). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-PHO%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R., Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
6 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
7 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
8 Wu C., Pike V.W., Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
9 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
10 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
11 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
12 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
13 Larbanoix, L., C. Burtea, S. Laurent, F. Van Leuven, G. Toubeau, L.V. Elst, and R.N. Muller, Potential amyloid plaque-specific peptides for the diagnosis of Alzheimer's disease. Neurobiol Aging, 2008